# ^18^F-Labeled 6-methyl-2-(4’-fluorophenyl)-1,3-benzothiazole

Chemical name: | ^18^F-Labeled 6-methyl-2-(4’-fluorophenyl)-1,3-benzothiazole | [image]
Abbreviated name: | [^18^F]5 | [image]
Synonym: | | [image]
Agent Category: | Compound | [image]
Target: | β-Amyloid plaques (Aβ) | [image]
Target Category: | Protein | [image]
Method of detection: | Positron emission tomography (PET) | [image]
Source of signal / contrast: | ^18^F | [image]
Activation: | No | [image]
Studies: | - In vitro; - Rodents | Structures of [^18^F]3a, [^18^F]3b and [^18^F]5.

## Background

[PubMed] (http://www.ncbi.nlm.nih.gov/pubmed?term=amyloid%20imaging%20agents&cmd=DetailsSearch)

Development of Alzheimer’s disease (AD) has been attributed to neurodegeneration as a result of the neuronal overexpression, secretion, and deposition of the neurotoxic amyloid β (Aβ) fragment of the Aβ protein precursor in the brain (1). No specific treatment for AD is currently available, and clinicians are increasingly focused on developing ways to either prevent or delay the formation of Aβ plaques in the brain of AD patients (2). In addition, several hundred clinical trials (http://clinicaltrials.gov/ct2/results?term=Alzheimer%E2%80%99s+disease+) approved by the United States Food and Drug Administration have been completed or are in progress to develop drugs for the prevention, onset delay, or treatment of AD. Early detection of Aβ plaques by non-invasive techniques such as positron emission tomography (PET) is often used to identify individuals who are prone to get the disease and to monitor the efficacy of drugs used to treat or delay onset of the disease (3). Although several immunohistochemical fluorescent stains and an antibody directed against the Aβ have been used to detect the plaques in the brain of AD patients, this information can be obtained only during postmortem (4). Hence, the development and evaluation of a suitable agent that can non-invasively detect Aβ plaques during early onset and monitor progression and treatment of the disease is an ongoing task.

Many radiolabeled tracers have been developed and evaluated under preclinical conditions, but among these only the ^11^C-labeled Pittsburgh compound B (6-hydroxy-2-(4’-N-[^11^C]methylaminophenyl)-1,3-benzothiazole ([^11^C]PIB (http://www.ncbi.nlm.nih.gov/bookshelf/br.fcgi?book=micad&part=PIB11C))) is the most commonly used PET tracer for detection of the Aβ plaques (3, 4). However, a major limitation of labeled compound is the short half-life (20.4 min) of ^11^C, which means that the use of [^11^C]PIB is restricted to clinical facilities that can generate the radionuclide on-site (3). To circumvent limitations observed with the ^11^C-labeled compounds, investigators developed several compounds labeled with ^18^F (half-life, 109.8 min) that can be used non-invasively with PET, but these tracers either have a low specificity or are still under clinical evaluation (5-7). In an effort to develop and evaluate radiotracers that can be used to detect and monitor the progression and treatment of AD, Serdons et al. (4) synthesized three benzothiazole derivatives, 6-methoxy-2-(4’-[^18^F]fluorophenyl)-1,3-benzothiazole ([^18^F]3a), 6-hydroxy-2-(4’-[^18^F]fluorophenyl)-1,3-benzothiazole ([^18^F]3b), and 6-methyl-2-(4’-[^18^F]fluorophenyl)-1,3-benzothiazole ([^18^F]5), and evaluated the affinity of these labeled compounds for Aβ fibrils under in vitro conditions. In addition, the biodistribution of these radiochemicals was studied in normal mice, and the brain pharmacokinetics of these labeled compounds were investigated in normal mice and rats using micro-PET (μPET).

### Other sources of information regarding human β amyloid protein

β Amyloid plaques in OMIM (http://www.ncbi.nlm.nih.gov/omim?term=Beta%20amyloid%20plaques) (Online Mendelian Inheritance in Man).

Human β amyloid protein (http://www.ncbi.nlm.nih.gov/protein/P05067.3?ordinalpos=3&itool=EntrezSystem2.PEntrez.Sequence.Sequence_ResultsPanel.Sequence_RVDocSum) and nucleotide (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=gene&Cmd=retrieve&dopt=full_report&list_uids=351&log$=databasead1&logdbfrom=nuccore) sequence.

Alzheimer’s disease in OMIM (http://www.ncbi.nlm.nih.gov/omim?term=Alzheimer%E2%80%99s%20disease%20).

Alzheimer’s disease in Genome Wide Association Studies (http://www.genome.gov/gwastudies/index.cfm?#searchForm) database.

FDA-approved treatments (http://www.alz.org/national/documents/topicsheet_treatments.pdf) for Alzheimer’s disease (from Alzheimer’s Association web site; www.alz.org).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=6-methyl-2-%284-fluorophenyl%29-1%2C3-benzothiazole&cmd=DetailsSearch)]

The synthesis processes of [^18^F]3a (6-methoxy-2-(4’-[^18^F]fluorophenyl)-1,3-benzothiazole), [^18^F]3b (6-hydroxy-2-(4’-[^18^F]fluorophenyl)-1,3-benzothiazole), and [^18^F]5 (6-methyl-2-(4’-[^18^F]fluorophenyl)-1,3-benzothiazole) were described by Serdons et al. (4). The decay-corrected radiochemical yields of these tracers were 24.1 ± 2.3%, 38.0 ± 0.2%, and 29.4 ± 3.2%, respectively. The time of synthesis required to obtain the labeled product was 60–80 min. The identity of each compound was confirmed by co-injection and co-elution with a corresponding nonradioactive sample of the compound using analytical reverse-phase high-performance liquid chromatography (RP-HPLC). The purity of each radiolabeled compound was reported to be >95% as determined with RP-HPLC. The average specific activity of the radiolabeled compounds at the end of synthesis was 116 GBq/μmol (3.13 Ci/μmol) (4).

Details of the biostability of [^18^F]5 in the plasma of mice and the brains of mice and rats (4) are provided in the appropriate Animal Studies subsections below.

[^11^C]PIB used for comparison purposes was synthesized as described elsewhere (8), but the radiochemical yield, purity, and specific activity of the radiocompound were not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=6-methyl-2-%284-fluorophenyl%29-1%2C3-benzothiazole%20in%20vitro&cmd=DetailsSearch)]

The affinities of nonradioactive compounds 3a, 3b, 5, and [^11^C]PIB for Aβ plaques, using human AD brain homogenates in a [^125^I]IMPY binding competition assay, were reported to be 2.2 ± 0.5, 22.5 ± 4.5, 5.7 ± 1.8, and 2.8 ± 0.5 nM, respectively (4). This indicated that compound 3b had a low affinity for the Aβ plaques, but the affinities of 3a and 5 were comparable to that of [^11^C]PIB.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=6-methyl-2-%284-fluorophenyl%29-1%2C3-benzothiazole%20and%20rodentia&cmd=DetailsSearch)]

The biodistribution of [^18^F]3a, [^18^F]3b, [^18^F]5, and [^11^C]PIB was studied in male NMRI mice (n = 4–6 animals/time point per radiotracer) at 2 min and 60 min after an injection through the tail vein (4). The animals were euthanized at the appropriate time point, and the various organs were removed and counted for accumulated radioactivity. Data obtained from the study were presented either as percentage of injected dose (% ID) or as % ID per gram tissue (% ID/g). For details of the biodistribution study, see Tables 2, 3, 4, and 5 in Serdons et al. (4). Also, only data for the brain are considered here because accumulation of radioactivity in the other organs is of little consequence when detecting Aβ plaques. Briefly, the initial uptake values of [^18^F]3a (5.1 ± 0.4% ID/g) and [^18^F]5 (5.3 ± 0.7% ID/g) were slightly higher than that of [^18^F]3b (4.7 ± 0.5% ID/g). Also, [^18^F]5 had a significantly higher (P < 0.05, two-sided) uptake at 2 min postinjection (p.i.) compared with [^11^C]PIB (3.6 ± 1.4% ID/g). The brain washout (ratio of % ID in cerebrum at 2 min to % ID in cerebrum at 60 min) of [^18^F]5 was higher (ratio = 23.1) than either [^18^F]3a (ratio = 12.1) or [^18^F]3b (ratio = 8.4), and this value was almost four-fold higher than that of [^11^C]PIB (ratio = 6.0), indicating that [^18^F]5 could be a promising agent for imaging Aβ plaques under in vivo conditions (4). The clearance from the blood (ratio of % ID in blood at 2 min to % ID in blood at 60 min) of [^18^F]5 (ratio = 2.0) was between that of [^18^F]3a (ratio = 1.1) and those of [^18^F]3b (ratio = 3.0) and [^11^C]PIB (ratio = 2.9). Radioactivity derived from the various labeled compounds was eliminated from the animals primarily through the hepatobiliary system (range, 48–71% ID) and to some extent through the urine (range, 5.6–26% ID).

Because [^18^F]5 showed superior uptake and washout characteristics in the brain of normal mice compared to the other ^18^F-labeled compounds, Serdons et al. investigated the stability of this radiochemical in the plasma and brain of these animals (4). The animals (n = 3 mice/time point) were injected with the tracer through the tail vein and killed by decapitation at 2, 10, 30, or 60 min p.i. Plasma from the animals was recovered and analyzed with RP-HPLC after co-injection with a nonradioactive sample of compound 5. Only 60% of the labeled compound remained intact at 2 min, and at least three unidentified metabolites of [^18^F]5 were detected. By 60 min p.i., only 1.6% of [^18^F]5 was intact in the plasma versus 80% of [^11^C]PIB. In the mouse brain, <15% of [^18^F]5-labeled metabolites were observed at either 2 min or 60 min p.i., indicating that little metabolism of the radiolabeled compound occurred in this organ and that the radiometabolites did not cross the blood–brain barrier in these animals (4). In another study using the rat (n = 1), ~80% of [^18^F]5 was reported to remain intact in the brain of this animal at 2 min p.i. (data at 60 min p.i. for this animal were not reported), which was comparable to the degree of breakdown observed for [^11^C]PIB in these animals.

The brain pharmacokinetics of [^18^F]3a, [^18^F]3b, and [^18^F]5 were compared using μPET to those of [^11^C]PIB in a normal rat (4). The respective tracers were administered to the animal (under anesthesia, but breathing spontaneously) through the tail vein with a time period of 5 d between each injection of ^18^F-labeled compound. Dynamic μPET images were acquired for 120 min after the injection of each radiochemical. The data with [^11^C]PIB (acquired for 90 min), for comparison with the ^18^F tracers, were obtained during a μPET study performed with the same rat 2 weeks earlier. All data were expressed as standard uptake values. All the radioactive compounds, including [^11^C]PIB, had a similar rapid brain uptake and a fast clearance profile compared to the variable uptake and clearance rates observed for these radiochemicals in the mouse brain during the biodistribution studies. The differences in uptake and washout observed between the rat and mouse brain were attributed to interspecies characteristics of the animals (4). Because no ^18^F was detected in the skull of the rat during the μPET study, the investigators concluded that little or no defluorination of the labeled 2-phenylbenzothiazoles was apparent under in vivo conditions.

With results obtained from these studies, the investigators concluded that [^18^F]5 could be a suitable compound for the detection of Aβ plaques in human AD patients (4). However, it is important to mention that [^18^F]5 would have to be evaluated in clinical trials before it can be used for the intended purpose in humans.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=6-methyl-2-%284-fluorophenyl%29-1%2C3-benzothiazole%20Non-Primate%20Mammals&cmd=DetailsSearch)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28primate%20NOT%20human%29)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=6-methyl-2-%284-fluorophenyl%29-1%2C3-benzothiazole%20Human%20Studies&cmd=DetailsSearch)]

No references are currently available.

## Supplemental Information

[Disclaimers]

No information is currently available.

## References

1 Bissette G. (2009). Does Alzheimer's disease result from attempts at repair or protection after transient stress?. J Alzheimers Dis.
2 Sano M., Grossman H., Van Dyk K. (2008). Preventing Alzheimer's disease : separating fact from fiction. CNS Drugs.
3 Serdons K., Van Laere K., Janssen P., Kung H.F., Bormans G., Verbruggen A. (2009). Synthesis and evaluation of three 18F-labeled aminophenylbenzothiazoles as amyloid imaging agents. J Med Chem.
4 Serdons K., Terwinghe C., Vermaelen P., Van Laere K., Kung H., Mortelmans L., Bormans G., Verbruggen A. (2009). Synthesis and Evaluation of (18)F-Labeled 2-Phenylbenzothiazoles as Positron Emission Tomography Imaging Agents for Amyloid Plaques in Alzheimer's Disease. J Med Chem.
5 Koole M., Lewis D.M., Buckley C., Nelissen N., Vandenbulcke M., Brooks D.J., Vandenberghe R., Van Laere K. (2009). Whole-body biodistribution and radiation dosimetry of 18F-GE067: a radioligand for in vivo brain amyloid imaging. J Nucl Med.
6 Nelissen N., Van Laere K., Thurfjell L., Owenius R., Vandenbulcke M., Koole M., Bormans G., Brooks D.J., Vandenberghe R. (2009). Phase 1 study of the Pittsburgh compound B derivative 18F-flutemetamol in healthy volunteers and patients with probable Alzheimer disease. J Nucl Med.
7 Rowe C.C., Ackerman U., Browne W., Mulligan R., Pike K.L., O'Keefe G., Tochon-Danguy H., Chan G., Berlangieri S.U., Jones G., Dickinson-Rowe K.L., Kung H.P., Zhang W., Kung M.P., Skovronsky D., Dyrks T., Holl G., Krause S., Friebe M., Lehman L., Lindemann S., Dinkelborg L.M., Masters C.L., Villemagne V.L. (2008). Imaging of amyloid beta in Alzheimer's disease with 18F-BAY94-9172, a novel PET tracer: proof of mechanism. Lancet Neurol.
8 Solbach C., Uebele M., Reischl G., Machulla H.J. (2005). Efficient radiosynthesis of carbon-11 labelled uncharged Thioflavin T derivatives using [11C]methyl triflate for beta-amyloid imaging in Alzheimer's Disease with PET. Appl Radiat Isot.